# ^64^Cu-1,4,7,10-Tetraazacyclododecane-1,4,7,10-tetraacetic acid-epidermal growth factor receptor-binding fibronectin domain E13.4.3'

Chemical name: | ^64^Cu-1,4,7,10-Tetraazacyclododecane-1,4,7,10-tetraacetic acid-EGFR-binding fibronectin domain E13.4.3'
Abbreviated name: | ^64^Cu-DOTA-Fn_E13.4.3'_, ^64^Cu-Fn_E13.4.3'_
Synonym:
Agent category: | Protein
Target: | Epidermal growth factor receptor (EGFR, HER1)
Target category: | Receptor
Method of detection: | Positron emission tomography (PET)
Source of signal: | ^64^Cu
Activation: | No
Studies: | - In vitro; - Rodents | Click on protein (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=protein&val=5725426), nucleotide (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=nucleotide&val=31406) (RefSeq), and gene (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?db=gene&cmd=Retrieve&dopt=full_report&list_uids=407105) for more information about fibronectin.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Copper%2064-Fn%20and%20human)]

Epidermal growth factor (EGF) is a 53-amino-acid growth factor (6.2 kDa) that is secreted by ectodermic cells, monocytes, kidneys, and duodenal glands (1). EGF stimulates the growth of epidermal and epithelial cells. EGF and at least seven other growth factors and their transmembrane receptor kinases play important roles in cell proliferation, survival, adhesion, migration, and differentiation. The EGF receptor (EGFR) family consists of four transmembrane receptors, including EGFR (HER1/erbB-1), HER2 (erbB-2/neu), HER3 (erbB-3), and HER4 (erbB-4) (2). HER1, HER3, and HER4 comprise three major functional domains: an extracellular ligand-binding domain, a hydrophobic transmembrane domain, and a cytoplasmic tyrosine kinase domain. No ligand has been clearly identified for HER2; however, HER2 can be activated as a result of ligand binding to other HER receptors with the formation of receptor homodimers and/or heterodimers (3). HER1 as well as HER2 are overexpressed on many solid tumor cells such as breast, non–small-cell lung, head and neck, and colon cancers (4-6). The high levels of HER1 and HER2 expression on cancer cells are associated with poor patient prognosis because high levels are related to increased proliferation (7-10).

Trastuzumab, a humanized immunoglobulin G_1_ (IgG_1_) monoclonal antibody (mAb) against the extracellular domain of recombinant HER2 (11), was labeled as ^111^In-trastuzumab (12-14). C225, an anti-EGFR (HER1), mouse-human chimeric, IgG_1_ mAb, also known as erbitux and cetuximab, was labeled as ^99m^Tc-EC-C225 (http://www.ncbi.nlm.nih.gov/books/NBK23305/) (15, 16) and ^64^Cu-DOTA-cetuximab (http://www.ncbi.nlm.nih.gov/books/NBK23434/) for imaging EGFR expression on solid tumors with the use of single-photon emission computed tomography (SPECT) and positron emission tomography (PET), respectively. However, the pharmacokinetics of the intact radiolabeled mAb, with high liver uptake and slow blood elimination, are generally not ideal for imaging (17, 18). Smaller antibody fragments, such as scFv, Fab, or F(ab')_2_, have better imaging pharmacokinetics because they are rapidly excreted by the kidneys. Nanobodies (15 kDa) and affibodies (50 kDa) exhibit efficient and specific tumor targeting but with high kidney accumulation (19-21). An engineered fibronectin scaffold with EGFR-binding domain (Fn_E13.4.3'_, 10 kDa) was radiolabeled with ^64^Cu via 1,4,7,10-tetraazacyclododecane-1,4,7,10-tetraacetic acid (DOTA) conjugation to form ^64^Cu-DOTA-Fn_E13.4.3'_ as a PET probe for in vivo imaging of EGFR in tumor-bearing nude mice (22). Fn_E13.4.3'_ does not contain the integrin binding sequence of Arg-Gly-Asp (RGD) (23).

### Related Resource Links:

- Chapters in MICAD (EGFR (http://www.ncbi.nlm.nih.gov/sites/entrez?db=Books&cmd=Search&term=HER1+AND+micad%5bbook%5d&doptcmdl=TOCView&log%24=booksrch&bname=micad))
- Gene information in NCBI (EGFR (http://www.ncbi.nlm.nih.gov/gene/1956), fibronectin (http://www.ncbi.nlm.nih.gov/gene/2335))
- Articles in Online Mendelian Inheritance in Man (OMIM) (EGFR (http://www.ncbi.nlm.nih.gov/omim/131550), fibronectin (http://omim.org/entry/135600))
- Clinical trials (trastuzumab (http://www.clinicaltrials.gov/ct2/results?term=Trastuzumab), cetuximab (http://www.clinicaltrials.gov/ct2/results?term=Cetuximab))
- Drug information in FDA (trastuzumab (http://google2.fda.gov/search?q=Trastuzumab&client=FDAgov&site=FDAgov&lr=&proxystylesheet=FDAgov&output=xml_no_dtd&getfields=*&x=11&y=14), cetuximab (http://google2.fda.gov/search?q=Cetuximab&client=FDAgov&site=FDAgov&lr=&proxystylesheet=FDAgov&output=xml_no_dtd&getfields=*&x=7&y=18))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Copper%2064-Fn%20and%20synthesis)]

EGFR-binding Fn_E13.4.3'_ (92 amino acids) with amino acid residue 63 mutated to arginine to create a single primary amine at the N-terminus was purified from the transfected bacteria (22). A C-terminal His_6_ tag was added for purification and identification. DOTA-Fn_E13.4.3'_ was prepared by incubation of Fn_E13.4.3'_ and DOTA-N-hydroxysuccinimide ester in 1:20 molar ratio for 60 min at room temperature. DOTA-Fn_E13.4.3'_ was purified with high-performance liquid chromatography and mass spectroscopy analysis supported a 1:1 DOTA to protein conjugation. Radiolabeling was performed by mixing ^64^CuCl_2_ with DOTA- Fn_E13.4.3'_ in sodium acetate buffer at pH 5.5. The mixture was heated at 37°C for 60 min. ^64^Cu-DOTA-Fn_E13.4.3'_ was purified with column chromatography. The radiochemical purity was >96%, with a specific activity of 15 MBq/nmol (0.41 mCi/nmol) at the end of purification. The labeling yield was ~90%. ^64^Cu-DOTA-Fn_E13.4.3'_ was >98% intact in 50% human or mouse serum at 37°C for 24 h. EGFR non-binding ^64^Cu-DOTA-Fn_WT'_ was also prepared similarly.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Copper%2064-Fn%20and%20in%20vitro)]

^64^Cu-DOTA-Fn_E13.4.3'_ (40 nM) exhibited significantly higher accumulation of radioactivity in EGFR(+) A431 human epidermoid carcinoma cells than ^64^Cu-DOTA-Fn_WT'_ and buffer (P < 0.005) (22). Unlabeled Fn_E13.4.3'_ (800 nM) blocked the accumulation by >65% (P < 0.03). Using five cell lines with different expression levels of EGFR for ^64^Cu-DOTA-Fn_E13.4.3'_ binding, there was significant correlation between ^64^Cu-DOTA-Fn_E13.4.3’'_ accumulation and EGFR expression levels (P < 0.017). Saturation binding assays showed the binding affinity (K_d_) values were 5 ± 2 nM and 17 ± 10 nM for Fn_E13.4.3'_ and DOTA-Fn_E13.4.3'_, respectively.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Copper%2064-Fn%20and%20rodentia)]

Hackel et al. (22) performed ex vivo biodistribution studies of 1 MBq (0.03 mCi) ^64^Cu-DOTA-Fn_E13.4.3'_ (0.25 nmol) or 1 MBq (0.03 mCi) ^64^Cu-DOTA-Fn_WT'_ (0.1 nmol) in A431 tumor-bearing nude mice (n = 3) at 1 h after injection. Accumulation of ^64^Cu-DOTA-Fn_E13.4.3'_ into A431 tumor was 2.4 ± 1.0% injected dose/gram (ID/g). The kidney accumulation was 200% ID/g. The accumulation levels in other normal tissues were low (<1% ID/g) except those for the liver (3% ID/g) and lung (7% ID/g). The tumor/blood and tumor/muscle ratios were 8.9 and 10.3, respectively. ^64^Cu-DOTA-Fn_WT'_ showed low accumulation in the tumor (0.6 ± 0.1% ID/g) but a similar biodistribution profile in the non-tumor tissues. No blocking studies were performed with unlabeled Fn_E13.4.3'_.

Whole-body PET imaging studies were performed in A431 or MDA-MB-435 tumor-bearing nude mice at 1, 2, 4, and 24 h after injection of 1 MBq (0.03 mCi) ^64^Cu-DOTA-Fn_E13.4.3'_ (n = 5) or 1 MBq (0.03 mCi) ^64^Cu-DOTA-Fn_WT'_ (n = 3) (22). The A431 tumor was clearly visualized with ^64^Cu-DOTA-Fn_E13.4.3'_ but not with ^64^Cu-DOTA-Fn_WT'_ at 1 h after injection. Tumor accumulation level (estimated from the PET images) of ^64^Cu-DOTA-Fn_E13.4.3'_ was 3.4 ± 1.0% ID/g at 1 h with a tumor/muscle ratio of 8.6. At 24 h, the tumor accumulation level of ^64^Cu-DOTA-Fn_E13.4.3'_ was 2.7 ± 0.6% ID/g with a tumor/muscle ratio of 6.9. Tumor accumulation level of ^64^Cu-DOTA-Fn_WT'_ was 0.8 ± 0.2% ID/g at 1 h with a tumor/muscle ratio of 1.8. Intense accumulation in the kidneys and urinary bladder was observed. ^64^Cu-DOTA-Fn_E13.4.3'_ exhibited <1% ID/g in MDA-MB-435 tumors (low EGFR expression). No blocking studies were performed.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Copper%2064-Fn%20and%20%28dog%20or%20pig%20or%20sheep%20or%20rabbit%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Copper%2064-Fn%20and%20%28primate%20not%20human%29)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Copper%2064-Fn%20and%20human)]

No publication is currently available.

## References

1 Carpenter G., Cohen S. (1990). Epidermal growth factor. J Biol Chem.
2 Yarden Y. (2001). The EGFR family and its ligands in human cancer: signalling mechanisms and therapeutic opportunities. Eur J Cancer.
3 Rubin I., Yarden Y. (2001). The basic biology of HER2. Ann Oncol.
4 Grunwald V., Hidalgo M. (2003). Developing inhibitors of the epidermal growth factor receptor for cancer treatment. J Natl Cancer Inst.
5 Mendelsohn J. (1990). Anti-epidermal growth factor receptor monoclonal antibodies as potential anti-cancer agents. J Steroid Biochem Mol Biol.
6 Yasui W., Sumiyoshi H., Hata J., Kameda T., Ochiai A., Ito H., Tahara E. (1988). Expression of epidermal growth factor receptor in human gastric and colonic carcinomas. Cancer Res.
7 Ang K.K., Berkey B.A., Tu X., Zhang H.Z., Katz R., Hammond E.H., Fu K.K., Milas L. (2002). Impact of epidermal growth factor receptor expression on survival and pattern of relapse in patients with advanced head and neck carcinoma. Cancer Res.
8 Costa S., Stamm H., Almendral A., Ludwig H., Wyss R., Fabbro D., Ernst A., Takahashi A., Eppenberger U. (1988). Predictive value of EGF receptor in breast cancer. Lancet.
9 Ethier S.P. (1995). Growth factor synthesis and human breast cancer progression. J Natl Cancer Inst.
10 Yarden Y. (2001). Biology of HER2 and its importance in breast cancer. Oncology.
11 Carter P., Presta L., Gorman C.M., Ridgway J.B., Henner D., Wong W.L., Rowland A.M., Kotts C., Carver M.E., Shepard H.M. (1992). Humanization of an anti-p185HER2 antibody for human cancer therapy. Proc Natl Acad Sci U S A.
12 Perik P.J., Lub-De Hooge M.N., Gietema J.A., van der Graaf W.T., de Korte M.A., Jonkman S., Kosterink J.G., van Veldhuisen D.J., Sleijfer D.T., Jager P.L., de Vries E.G. (2006). Indium-111-labeled trastuzumab scintigraphy in patients with human epidermal growth factor receptor 2-positive metastatic breast cancer. J Clin Oncol.
13 Lub-de Hooge M.N., Kosterink J.G., Perik P.J., Nijnuis H., Tran L., Bart J., Suurmeijer A.J., de Jong S., Jager P.L., de Vries E.G. (2004). Preclinical characterisation of 111In-DTPA-trastuzumab. Br J Pharmacol.
14 Garmestani K., Milenic D.E., Plascjak P.S., Brechbiel M.W. (2002). A new and convenient method for purification of 86Y using a Sr(II) selective resin and comparison of biodistribution of 86Y and 111In labeled Herceptin. Nucl Med Biol.
15 Schechter N.R., Yang D.J., Azhdarinia A., Kohanim S., Wendt R., Oh C.S., Hu M., Yu D.F., Bryant J., Ang K.K., Forster K.M., Kim E.E., Podoloff D.A. (2003). Assessment of epidermal growth factor receptor with 99mTc-ethylenedicysteine-C225 monoclonal antibody. Anticancer Drugs.
16 Schechter N.R., Wendt R.E., Yang D.J., Azhdarinia A., Erwin W.D., Stachowiak A.M., Broemeling L.D., Kim E.E., Cox J.D., Podoloff D.A., Ang K.K. (2004). Radiation dosimetry of 99mTc-labeled C225 in patients with squamous cell carcinoma of the head and neck. J Nucl Med.
17 Olafsen T., Wu A.M. (2010). Antibody vectors for imaging. Semin Nucl Med.
18 Wu A.M. (2009). Antibodies and antimatter: the resurgence of immuno-PET. J Nucl Med.
19 Arbabi Ghahroudi M., Desmyter A., Wyns L., Hamers R., Muyldermans S. (1997). Selection and identification of single domain antibody fragments from camel heavy-chain antibodies. FEBS Lett.
20 Desmyter A., Decanniere K., Muyldermans S., Wyns L. (2001). Antigen specificity and high affinity binding provided by one single loop of a camel single-domain antibody. J Biol Chem.
21 Muyldermans S. (2001). Single domain camel antibodies: current status. J Biotechnol.
22 Hackel B.J., Kimura R.H., Gambhir S.S. (2012). Use of (64)Cu-labeled fibronectin domain with EGFR-overexpressing tumor xenograft: molecular imaging. Radiology.
23 Hackel B.J., Ackerman M.E., Howland S.W., Wittrup K.D. (2010). Stability and CDR composition biases enrich binder functionality landscapes. J Mol Biol.